# Cy5.5-GGPRQITAGK(Fitc)C-Poly-L-lysine-methoxypolyethylene glycol

Chemical name: | Cy5.5-Poly-L-lysine-methoxypolyethylene glycol
Abbreviated name: | Cy5.5-GGPRQITAGK(Fitc)C-PL-MPEG
Synonym:
Agent Category: | Peptide
Target: | Gelatinases (MMP-2 and MMP-9)
Target Category: | Enzyme binding
Method of detection: | Optical, near-infrared fluorescence
Source of signal/contrasat: | Cy5.5
Activation: | Yes
Studies: | - In vitro; - Rodents | Click on MMP-2 (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=116856) and MMP-9 (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=10443048) for protein information.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Poly-L-lysine+MPEG)]

Optical fluorescence imaging is increasingly used to study biological functions of specific targets (1, 2). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–700 nm) are used. Near-infrared (NIR) fluorescence (650–900 nm) detection avoids the background fluorescence interference of natural biomolecules, providing a high contrast between target and background tissues. NIR fluorophores have wider dynamic range and minimal background as a result of reduced scattering compared with visible fluorescence detection. They also have high sensitivity, resulting from low infrared background, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is becoming a non-invasive alternative to radionuclide imaging in small animals.

Extracellular matrix (ECM) adhesion molecules consist of a complex network of fibronectins, collagens, chondroitins, laminins, glycoproteins, heparin sulfate, tenascins, and proteoglycans that surround connective tissue cells, and they are mainly secreted by fibroblasts, chondroblasts, and osteoblasts (3). Cell substrate adhesion molecules are considered essential regulators of cell migration, differentiation, and tissue integrity and remodeling. These molecules play a role in inflammation and atherogenesis, but they also participate in the process of invasion and metastasis of malignant cells in the host tissue (4). Invasive tumor cells adhere to the ECM, which provides a matrix environment for permeation of tumor cells through the basal lamina and underlying interstitial stroma of the connective tissue. Overexpression of matrix metalloproteinases (MMPs) and other proteases by tumor cells allows intravasation of tumor cells into the circulatory system after degrading the basement membrane and ECM (5).

Several families of proteases are involved in atherogenesis, myocardial infraction, angiogenesis, and tumor invasion and metastases (6-9). The gelatinase family is a subgroup of MMPs consisting of gelatinase A (MMP-2) and gelatinase B (MMP-9) (10). Gelatinase expression in normal cells, such as trophoblasts, osteoclasts, neutrophils, and macrophages, is highly regulated. Elevated levels of gelatinases have been found in tumors that are associated with a poor prognosis for cancer patients (11). A synthetic protected graft copolymer (PGC) consisting of poly-L-lysine (PL) with multiple methoxypolyethylene glycol (MPEG) side chains has been used as a drug carrier with efficient accumulation in tumors (12, 13). A peptide, GGPRQITAG, was found to be a MMP-2/9 substrate from a phage library and is cleaved between Gln (Q) and Ile (I) residues (14). Chen et al. (15) used this sequence with linking residues GGPRQITAGK(Fitc)C with a Cy5.5 NIR dye molecule to attach to the unmodified PL side chains to form a fluorescence-quenched polymer, Cy5.5-GGPRQITAGK(Fitc)C-PL-MPEG (Cy5.5-MMP-PGC). The Cy5.5 molecules are in close proximity, which results in fluorescence quenching because of efficient fluorescence resonance energy transfer. The NIR fluorescence signal will increase when the Gln-Ile bond is cleaved by MMP-2/9, releasing fragments that contain Cy5.5. Cy5.5 is a NIR fluorescence dye with an absorbance maximum at 675 nm and an emission maximum at 694 nm with a high extinction coefficient of 250,000 M^-1^cm^-1^. Cy5.5-MMP-PGC is being developed for NIR fluorescence imaging of MMP-2/9 proteolytic activity in tumors, atherosclerosis, myocardial infarction, and other diseases (15, 16).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Poly-L-lysine+MPEG+synthesis)]

PL-MPEG was formed by a reaction of the hydroxysuccinimide ester of methoxypolyethylene glycol succinate to the ω-NH_2_ group of PL (35.5 kDa) (17). The purified PL-MPEG had a calculated average molecular mass of 480 kDa as determined with elemental analysis. The PL-MPEG was then iodoacetylated by reaction with excess iodoacetic acid (15, 16). GGPRQITAGK(Fitc)C was coupled to the iodoacetylated PL-MPEG via a thiol-specific reaction at the C-terminal amino acid (C). The resulting PGC was further modified with Cy5.5-hydroxysuccinimide ester via the free N-terminal amino acid (G) of the attached peptide. Cy5.5-MMP-PGC was purified with column chromatography. Each PL backbone contained an average of 92 MPEG molecules, 40 copies of MMP peptides, and 24 molecules of Cy5.5.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Poly-L-lysine+MPEG+and+in+vitro)]

Chen et al. (15) showed that Cy5.5-MMP-PGC (200 nM) was activated by MMP-2/9 (5 μg) in a time-dependent manner with a 200-fold increase in NIR fluorescence signal after 300 min of incubation. Deguchi et al. (16) showed that apolipoprotein E–deficient (apoE^-/-^) aortas without Cy5.5-MMP-PGC provided negligible NIR fluorescence signals, whereas the probe showed substantial signals. Pretreatment with a cyclic peptide gelatinase-selective inhibitor (200 nM) markedly reduced NIR fluorescence signal.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Poly-L-lysine+MPEG+rodentia)]

Chen et al. (15) performed fluorescence imaging studies of Cy5.5-MMP-PGC in mice at various time points up to 4 weeks after myocardial infarction induced by ligation of the left anterior descending coronary artery. Images were obtained after injection of 4 nmol Cy5.5-MMP-PGC. Substantial contrasts were observed between the infarcted area and normal tissue at 4 days with a maximum NIR fluorescence intensity at 1 week, followed by gradual decrease in signals at 2, 3, and 4 weeks. Zymography and real-time polymerase chain reaction experiments showed that MMP9 expression was increased at 2–4 days, and MMP2 expression was increased at 1–2 weeks. Immunofluorescence was colocalized with immunoreactivity for neutrophils and CD45, a leukocyte marker. No blocking or MMP inhibition experiment was performed.

Deguchi et al. (16) performed in vivo imaging of atherosclerosis in apoE^-/-^ mice using Cy5.5-PGC fluorescence-mediated tomography. Marked fluorescence signal could be detected in the aortic arch and abdominal aorta of the apoE^-/-^ mice 24 h after injection of 5 nmol of Cy5.5-PGC. Ex vivo imaging showed that the NIR fluorescence signal intensity was higher in the arch and abdominal aortic lesions of apoE^-/-^ mice compared with the unaffected aorta of control wild-type mice (P < 0.001). MMP immunohistochemistry and in situ zymography confirmed that the overexpression of gelatinolytic activity colocalized with NIR signal in the lesions. Furthermore, immunofluorescence also colocalized with immunoreactivity for Mac-3, a macrophage marker. No blocking or MMP inhibition experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Poly-L-lysine+MPEG+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Poly-L-lysine+MPEG+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Poly-L-lysine+MPEG+human)]

No publication is currently available.

## NIH Support

R01 CA74424-01

## References

1 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
2 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
3 Bosman F.T., Stamenkovic I. (2003). Functional structure and composition of the extracellular matrix. J Pathol.
4 Jiang W.G., Puntis M.C., Hallett M.B. (1994). Molecular and cellular basis of cancer invasion and metastasis: implications for treatment. Br J Surg.
5 Albelda S.M. (1993). Role of integrins and other cell adhesion molecules in tumor progression and metastasis. Lab Invest.
6 Keppler D., Sameni M., Moin K., Mikkelsen T., Diglio C.A., Sloane B.F. (1996). Tumor progression and angiogenesis: cathepsin B & Co. Biochem Cell Biol.
7 Liu J., Sukhova G.K., Sun J.S., Xu W.H., Libby P., Shi G.P. (2004). Lysosomal cysteine proteases in atherosclerosis. Arterioscler Thromb Vasc Biol.
8 Berchem G., Glondu M., Gleizes M., Brouillet J.P., Vignon F., Garcia M., Liaudet-Coopman E. (2002). Cathepsin-D affects multiple tumor progression steps in vivo: proliferation, angiogenesis and apoptosis. Oncogene.
9 Brix K., Dunkhorst A., Mayer K., Jordans S. (2007). and Cysteine cathepsins: Cellular roadmap to different functions. Biochimie.
10 Nelson A.R., Fingleton B., Rothenberg M.L., Matrisian L.M. (2000). Matrix metalloproteinases: biologic activity and clinical implications. J Clin Oncol.
11 Deryugina E.I., Quigley J.P. (2006). Matrix metalloproteinases and tumor metastasis. Cancer Metastasis Rev.
12 Marecos E., Weissleder R., Bogdanov A. (1998). Antibody-mediated versus nontargeted delivery in a human small cell lung carcinoma model. Bioconjug Chem.
13 Weissleder R., Cheng H.C., Marecos E., Kwong K., Bogdanov A. (1998). Non-invasive in vivo mapping of tumour vascular and interstitial volume fractions. Eur J Cancer.
14 Kridel S.J., Chen E., Kotra L.P., Howard E.W., Mobashery S., Smith J.W. (2001). Substrate hydrolysis by matrix metalloproteinase-9. J Biol Chem.
15 Chen J., Tung C.H., Allport J.R., Chen S., Weissleder R., Huang P.L. (2005). Near-infrared fluorescent imaging of matrix metalloproteinase activity after myocardial infarction. Circulation.
16 Deguchi J.O., Aikawa M., Tung C.H., Aikawa E., Kim D.E., Ntziachristos V., Weissleder R., Libby P. (2006). Inflammation in atherosclerosis: visualizing matrix metalloproteinase action in macrophages in vivo. Circulation.
17 Weissleder R., Tung C.H., Mahmood U., Bogdanov A. (1999). In vivo imaging of tumors with protease-activated near-infrared fluorescent probes. Nat Biotechnol.